# 5-(5-(2-(2-(2-[^18^F]Fluoroethoxy)ethoxy)ethoxy)benzofuran-2-yl)-N-methylpyridin-2-amine

Chemical name: | 5-(5-(2-(2-(2-[^18^F]Fluoroethoxy)ethoxy)ethoxy)benzofuran-2-yl)-N-methylpyridin-2-amine
Abbreviated name: | [^18^F]FPYBF-2
Synonym:
Agent category: | Compound
Target: | Amyloid-beta peptide
Target category: | Acceptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FPHBF-2)]

Alzheimer's disease (AD) is a form of dementia with a gradual memory loss and a progressive decline in mental functions over time (1, 2). It is characterized pathologically by neuronal loss, extracellular senile plaques (aggregates of amyloid-β peptides consisting of 40–42 amino acids), and intracellular neurofibrillary tangles (filaments of microtubule-binding hyperphosphorylated protein tau) in the brain, especially in the hippocampus and associative regions of the cortex (3, 4). β-Amyloid peptides and tau proteins are implicated as the main causes of neuronal degeneration and cell death (5, 6).

Early diagnosis of AD is important for treatment consideration and disease management (7). Various β-amyloid imaging agents have been developed for magnetic resonance imaging (MRI), single-photon emission computed tomography, and positron emission tomography (PET) (8-13) as measures of the presence of plaque. The binding of different derivatives of Congo red, thioflavin, stibene, and aminonaphthalene has been studied in human post-mortem brain tissue and in transgenic mice. Of these analogs, 2-(1-(6-[(2-[^18^F]fluoroethyl)(methyl)amino]-2-naphthyl)ethylidene)malono nitrile ([^18^F]FDDNP) was studied in humans, and it showed more binding in the brains of patients with AD than in those of healthy people (14). However, [^18^F]FDDNP showed low signal/noise ratios for PET imaging because it is highly lipophilic. N-Methyl-[^11^C]-2-(4’-methylaminophenyl)-6-hydroxybenzothiasole, a β-amyloid binding compound based on a series of neutral thioflavin-T derivatives (15), was radiolabeled with the positron-emitting radionuclide ^11^C ([^11^C]6-OH-BTA-1 or [^11^C]PIB). [^11^C]6-OH-BTA-1 was found to be a promising imaging agent for senile plaques in the brain (10). 5-(5-(2-(2-(2-[^18^F]Fluoroethoxy)ethoxy)ethoxy)benzofuran-2-yl)-N,N-dimethylpyridin-2-amine benzenamine ([^18^F]FPYBF-1) was found to exhibit good initial uptake but slow washout from the brain in normal mice, and thus it is not suitable for imaging studies. Ono et al. (16) reported the development of the less lipophilic monomethylamino derivative of [^18^F]FPHBF-1, 5-(5-(2-(2-(2-[^18^F]fluoroethoxy)ethoxy)ethoxy)benzofuran-2-yl)-N-methylpyridin-2-amine ([^18^F]FPYBF-2) as a PET imaging agent for β-amyloid plaques in the brain.

### Related Resource Links:

- Chapters in MICAD (Amyloid (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=amyloid+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (Amyloid (http://www.ncbi.nlm.nih.gov/gene/351))
- Articles in Online Mendelian Inheritance in Man (OMIM) (Amyloid (http://www.ncbi.nlm.nih.gov/omim/?term=Amyloid))
- Clinical trials (Amyloid (http://www.clinicaltrials.gov/ct2/results?term=Amyloid))
- Drug information in FDA (Amyloid inhibitors (http://google2.fda.gov/search?q=Amyloid+inhibitor&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=16&y=16))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FPHBF-2%20and%20synthesis)]

[^18^F]FPYBF-2 was readily synthesized by standard ^18^F-fluorination of the N-BOC–protected mesylate derivative with [^18^F]KF/Kryptofix 2.2.2, for 5 min at 120°C and the subsequent acid hydrolysis with 10% HCl for 5 min at 120°C (16). [^18^F]FPYBF-2 was purified with high-performance liquid chromatography. Overall radiochemical yield was 52%, with a specific activity of 242 GBq/µmol (6.5 Ci/µmol) at the end of synthesis and a radiochemical purity of >99%. Total synthesis time was not reported. CLogP (lipophilicity) values were calculated to be 2.94 and 3.73 for [^18^F]FPYBF-2 and [^18^F]FPYBF-1, respectively.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FPHBF-2%20and%20in%20vitro)]

FPYBF-2 has a binding affinity (K_i_) value of 3.85 ± 0.23 nM for aggregated β-amyloid(1–42) peptide in competition with [^125^I]IMPY (16). [^18^F]FPYBF-2 bound to the cortex of post-mortem AD brain slices but not to control brain slices as visualized with in vitro autoradiography studies. The brains showed a distinctive labeling of β-amyloid plaques by co-staining with thioflavin-S. No such labeling and staining were observed in the control wild-type mice. No blocking studies were performed.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FPHBF-2%20and%20rodentia)]

[^18^F]FPYBF-2 (0.37 MBq (10 μCi)) was injected intravenously into normal male mice (n = 5/group) to study its accumulation in the brain and other organs/tissues at 2, 10, 30, and 60 min after injection (16). [^18^F]FPYBF-2 showed rapid penetration into the brain with 7.38 ± 0.84% injected dose (ID)/g at 2 min and a quick washout (3.15 ± 0.10% ID/g at 60 min). The brain_2min_/brain_60min_ value was 2.34. In comparison, [^18^F]FPYBF-1 exhibited a brain_2min_/brain_60min_ value of 2.11, which was slightly lower than that of [^18^F]FPYBF-2. The organs with the highest accumulation at 60 min after injection were the intestine (30.9% ID/g) and stomach (22.5% ID/g), followed by the liver (8.71% ID/g), kidney (3.70% ID/g), lung (2.88% ID/g), and heart (2.60% ID/g). The radioactivity levels at 60 min were 2.42% ID/g and 1.72% ID/g in the blood and bone, respectively. The bone radioactivity was 2.65% ID/g at 2 min. Ex vivo autoradiography studies of the brains of transgenic Tg2576 mice overexpressing β-amyloid plaques in the brain were performed after injection of [^18^F]FPYBF-2. The brains showed a distinctive labeling of β-amyloid plaques and co-staining with thioflavin-S. No such labeling and staining were observed in the control wild-type mice. No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FPHBF-2%20and%20%28dog%20or%20pig%20or%20cat%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FPHBF-2%20and%20primate%20not%20human)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FPHBF-2%20and%20humans)]

No publication is currently available.

## References

1 Forstl H., Kurz A. (1999). Clinical features of Alzheimer's disease. Eur Arch Psychiatry Clin Neurosci.
2 Heininger K. (2000). A unifying hypothesis of Alzheimer's disease. IV. Causation and sequence of events. Rev Neurosci.
3 Mirra S.S., Heyman A., McKeel D., Sumi S.M., Crain B.J., Brownlee L.M., Vogel F.S., Hughes J.P., van Belle G., Berg L. (1991). The Consortium to Establish a Registry for Alzheimer's Disease (CERAD). Part II. Standardization of the neuropathologic assessment of Alzheimer's disease. Neurology.
4 Hardy J.A., Higgins G.A. (1992). Alzheimer's disease: the amyloid cascade hypothesis. Science.
5 Hardy J. (2003). The relationship between amyloid and tau. J Mol Neurosci.
6 Brandt R., Hundelt M., Shahani N. (2005). Tau alteration and neuronal degeneration in tauopathies: mechanisms and models. Biochim Biophys Acta.
7 de Leon M.J., DeSanti S., Zinkowski R., Mehta P.D., Pratico D., Segal S., Clark C., Kerkman D., DeBernardis J., Li J., Lair L., Reisberg B., Tsui W., Rusinek H. (2004). MRI and CSF studies in the early diagnosis of Alzheimer's disease. J Intern Med.
8 Bacskai B.J., Klunk W.E., Mathis C.A., Hyman B.T. (2002). Imaging amyloid-beta deposits in vivo. J Cereb Blood Flow Metab.
9 Nordberg A. (2004). PET imaging of amyloid in Alzheimer's disease. Lancet Neurol.
10 Klunk W.E., Engler H., Nordberg A., Wang Y., Blomqvist G., Holt D.P., Bergstrom M., Savitcheva I., Huang G.F., Estrada S., Ausen B., Debnath M.L., Barletta J., Price J.C., Sandell J., Lopresti B.J., Wall A., Koivisto P., Antoni G., Mathis C.A., Langstrom B. (2004). Imaging brain amyloid in Alzheimer's disease with Pittsburgh Compound-B. Ann Neurol.
11 Klunk W.E., Engler H., Nordberg A., Bacskai B.J., Wang Y., Price J.C., Bergstrom M., Hyman B.T., Langstrom B., Mathis C.A. (2003). Imaging the pathology of Alzheimer's disease: amyloid-imaging with positron emission tomography. Neuroimaging Clin N Am.
12 Wang Y., Klunk W.E., Debnath M.L., Huang G.F., Holt D.P., Shao L., Mathis C.A. (2004). Development of a PET/SPECT agent for amyloid imaging in Alzheimer's disease. J Mol Neurosci.
13 Kung M.P., Hou C., Zhuang Z.P., Skovronsky D., Kung H.F. (2004). Binding of two potential imaging agents targeting amyloid plaques in postmortem brain tissues of patients with Alzheimer's disease. Brain Res.
14 Shoghi-Jadid K., Small G.W., Agdeppa E.D., Kepe V., Ercoli L.M., Siddarth P., Read S., Satyamurthy N., Petric A., Huang S.C., Barrio J.R. (2002). Localization of neurofibrillary tangles and beta-amyloid plaques in the brains of living patients with Alzheimer disease. Am J Geriatr Psychiatry.
15 Bacskai B.J., Hickey G.A., Skoch J., Kajdasz S.T., Wang Y., Huang G.F., Mathis C.A., Klunk W.E., Hyman B.T. (2003). Four-dimensional multiphoton imaging of brain entry, amyloid binding, and clearance of an amyloid-beta ligand in transgenic mice. Proc Natl Acad Sci U S A.
16 Ono M., Cheng Y., Kimura H., Cui M., Kagawa S., Nishii R., Saji H. (2011). Novel (18)F-Labeled Benzofuran Derivatives with Improved Properties for Positron Emission Tomography (PET) Imaging of beta-Amyloid Plaques in Alzheimer's Brains. J Med Chem.